# (S)-5-Methoxymethyl-3-[6-(4,4,4-trifluorobutoxy)benzo[d]isoxazol-3-yl]-oxazolidin-2-[^11^C]one

Chemical name: | (S)-5-Methoxymethyl-3-[6-(4,4,4-trifluorobutoxy)benzo[d]isoxazol-3-yl]-oxazolidin-2-[^11^C]one
Abbreviated name: | [^11^C]SL25.1188
Synonym:
Agent category: | Compound
Target: | Monoamine oxidase B (MAO-B)
Target category: | Enzyme
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SL25.1188)]

Monoamine oxidase (MAO) is a mitochondrial enzyme that inactivates dopamine, noradrenaline, and serotonin in the brain (1, 2). Two isoforms, A and B, of the enzyme have been identified. MAO-A preferentially oxidizes serotonin and noradrenaline, whereas MAO-B preferentially oxidizes phenethylamine. Dopamine is a substrate for both enzymes. MAO-A is predominately associated with depression and anxiety disorders, whereas MAO-B is predominately associated with neurodegenerative diseases, such as Parkinson’s disease (PD), as indicated by studies with specific MAO isoform inhibitors (3-5). MAO-A is selectively inhibited by clorgyline, whereas MAO-B is selectively and irreversibly inhibited by L-depreny. In the human brain, MAO-B predominates and is present in both glial cells and neurons (6), most abundantly in serotonin and histamine neurons (7).

(S)-5-Methoxymethyl-3-[6-(4,4,4-trifluorobutoxy)-benzo[d]isoxazol-3-yl]-oxazolidin-2-one (SL25.1188) is a selective and reversible MAO-B inhibitor (8). For measurements of MAO-B activity, (S)-5-methoxymethyl-3-[6-(4,4,4-trifluorobutoxy)benzo[d]isoxazol-3-yl]-oxazolidin-2-[^11^C]one ([^11^C]SL25.1188) has been prepared for use in positron emission tomography (PET) studies.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=(MAO-A%20OR%20MAO-B)+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (MAO-B (http://www.ncbi.nlm.nih.gov/gene/4129)).
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/entrez/dispomim.cgi?cmd=entry&id=309860)
- Clinical trials (MAO-B (http://www.clinicaltrials.gov/ct2/results?term=MAO-B))
- Drug information in FDA (http://google2.fda.gov/search?q=MAO-B&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=9&y=10)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SL25.1188%20and%20synthesis)]

Saba et al. (8) reported the synthesis of [^11^C]SL25.1188 by cyclization reaction of [^11^C]phosgene with the corresponding ring-open precursor in CH_2_Cl_2_ (100°C for 2 min), with a radiochemical yield of ~7% (based on [^11^C]methane, decay-corrected) after purification with high-performance liquid chromatography (HPLC). The total synthesis time was 30–32 min, with a radiochemical purity of >95% and a specific activity of 50–70 GBq/μmol (1.35–1.89 Ci/μmol) at the end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SL25.1188%20and%20in%20vitro)]

SL25.1188 inhibited rat brain MAO-B with an 50% inhibitory concentration (IC_50_) value of 11.8 nM and an 84-fold selectivity over MAO-A (8).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SL25.1188%20and%20rodentia)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SL25.1188%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SL25.1188%20and%20%28primate%20not%20human%29)]

Saba et al. (8) performed PET imaging studies in four male baboons after injection of 88 MBq (2.4 mCi) [^11^C]SL25.1188. [^11^C]SL25.1188 exhibited a rapid phase of distribution in blood at 5 min after injection, followed by an elimination half-life of 85 ± 14 min. Plasma metabolism analysis with HPLC showed that no radioactive metabolite of [^11^C]SL25.1188 could be detected at 30 min. Brain accumulation was rapid with ~5% injected dose/100 ml. The highest regional brain accumulation (distribution volume (VT)) was observed in the thalamus (10.9), followed by the striatum (10.3), hippocampus (8.9), temporal cortex (7.7), parietal cortex (7.4), frontal cortex (7.4), white matter (7.4), occipital cortex (7.2), and pons (6.1). Pretreatment (30 min before the tracer injection) with deprenyl (2 mg/kg) or lazabemide (0.5 mg/kg) reduced VT values in all brain areas up to 50%. In displacement experiments (30 min after the tracer injection), injection of SL25.1188 (1 mg/kg) or deprenyl (2 mg/kg) strongly reduced the accumulation of [^11^C]SL25.1188 in all brain areas (85–100%) at 50 min after the inhibitor injection, while a lesser displacement was observed with lazabemide (0.5 mg/kg) (55–70%). Therefore, [^11^C]SL25.1188 binding to MAO-B in the brain is reversible.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SL25.1188%20and%20human)]

No publication is currently available.

## References

1 Richards J.G., Saura J., Ulrich J., Da Prada M. (1992). Molecular neuroanatomy of monoamine oxidases in human brainstem. Psychopharmacology (Berl).
2 Saura J., Kettler R., Da Prada M., Richards J.G. (1992). Quantitative enzyme radioautography with 3H-Ro 41-1049 and 3H-Ro 19-6327 in vitro: localization and abundance of MAO-A and MAO-B in rat CNS, peripheral organs, and human brain. J Neurosci.
3 Murphy D.L., Wyatt R.J. (1972). Reduced monoamine oxidase activity in blood platelets from schizophrenic patients. Nature.
4 Murphy D.L., Weiss R. (1972). Reduced monoamine oxidase activity in blood platelets from bipolar depressed patients. Am J Psychiatry.
5 Jarman J., Glover V., Sandler M., Turjanski N., Stern G. (1993). Platelet monoamine oxidase B activity in Parkinson's disease: a re-evaluation. J Neural Transm Park Dis Dement Sect.
6 Riederer P., Konradi C., Schay V., Kienzl E., Birkmayer G., Danielczyk W., Sofic E., Youdim M.B. (1987). Localization of MAO-A and MAO-B in human brain: a step in understanding the therapeutic action of L-deprenyl. Adv Neurol.
7 Vincent S.R. (1989). Histochemical localization of 1-methyl-4-phenyl-1,2,3,6-tetrahydropyridine oxidation in the mouse brain. Neuroscience.
8 Saba W., Valette H., Peyronneau M.A., Bramoulle Y., Coulon C., Curet O., George P., Dolle F., Bottlaender M. (2010). [(11)C]SL25.1188, a new reversible radioligand to study the monoamine oxidase type B with PET: preclinical characterisation in nonhuman primate. Synapse.